# Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-G3 nanoglobule-CGLIIQKNEC (CLT1)

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-G3 nanoglobule-CGLIIQKNEC (CLT1)
Abbreviated name: | Gd-DOTA-G3-CLT1
Synonym: | P-G3-Gd
Agent category: | Peptide
Target: | Fibrin-fibronectin clot complexes
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). A meshwork of clotted plasma protein was present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (4). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, they are largely nonspecific. CGLIIQKNEC (CLT1), a fibronectin-fibrin binding cyclic peptide, was identified with phage display screening (4). The peptide was conjugated with Gd-DTPA to form Gd-DTPA-CLT1 for imaging of fibronectin-fibrin complexes in tumor tissues showing specific accumulation in the tumors (7). Tan et al. (8) prepared a CLT1-targeted contrast agent (Gd-DOTA-G3-CLT1) with Gd-tetraazacyclododecane-1,4,7,10-tetraacetic acid (GD-DOTA)_43_ monoamide chelates and three CLT1 molecules conjugated to a generation 3 (G3) polylysine dendrimer with a cubic silsesquioxane core. Gd-DOTA-G3-CLT1 was evaluated as a MRI tumor contrast agent in nude mice bearing MDA-MB-231 human breast carcinoma xenografts.

### Related Resource Links:

- Chapters in MICAD (CLT1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CLT1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), fibronectin (http://omim.org/entry/135600))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+synthesis)]

CLT1 conjugate with polyethylene glycol (PEG)-propargyl group at the N-terminus was synthesized using solid-phase peptide synthesis (8). G3 nanoglobules were synthesized as previously described (9). G3 nanoglobules were activated with azido-dPEG N-hydroxysuccinimide for CTL1 conjugation and DOTA-tris(t-Bu) for Gd labeling. The G3 nanoglobule-(DOTA)_43_-(PEG-azido)_3_ conjugate was prepared with 60% yield, and its molecular weight was confirmed with mass spectroscopy. The G3 nanoglobule-(DOTA)_43_-(PEG-azido)_3_ conjugate (2 µmol) was incubated with four-fold excess Gd(OAc)_3_ at pH 6 for 48 h at room temperature. The product, G3 nanoglobule-(Gd-DOTA)_43_-(PEG-azido)_3_ conjugate, was purified with dialysis with 53% yield. G3 nanoglobule-(Gd-DOTA)_43_-(PEG-azido)_3_ conjugate (0.9 µmol), copper(II) sulfate (4 µmol), and CTL1-PEG-propargyl conjugate (8.1 µmol) were incubated for 24 h at room temperature. The final product, G3 nanoglobule-(Gd-DOTA)_43_-(CTL1)_3_ (Gd-DOTA-G3-CLT1) conjugate, was purified with ultrafiltration and dialysis with 78% yield, and its molecular weight was confirmed with mass spectroscopy. There were 43 Gd and 3 CTL1 moieties per G3 nanoglobule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+in+vitro)]

Gd-DOTA-G3-CLT1 exhibited r_1_ and r_2_ values of 8.20 mM^–1^s^–1^ per Gd and 16.10 mM^–1^s^–1^ per Gd at 3 T, respectively (8). Gd-DOTA-G3-CLT1 had a size of 6.2 nm as measured with dynamic laser scattering. Non-targeted Gd-DOTA-G3 exhibited r_1_ and r_2_ values of 8.03 mM^–1^s^–1^ per Gd and 16.40 mM^–1^s^–1^ per Gd at 3 T, respectively. Gd-DOTA-G3 had a size of 5.8 nm. Gd-DTPA-CLT1 exhibited T1 and T2 relaxivity values of 4.22 mM^–1^s^–1^ and 4.45 mM^–1^s^–1^ at 3 T, respectively (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+rodentia)]

Tan et al. (8) performed dynamic T1-weighted MRI (7 T) studies with intravenous injection of 0.03 mmol Gd/kg Gd-DOTA-G3-CLT1 in female nude mice (n = 3) bearing MDA-MB-231 xenografts. Gd-DOTA-G3 (0.03 mmol Gd/kg) was used a control contrast agent. Contrast-enhanced MRI images were obtained before injection and at 2, 5, 10, 15, 30, and 60 min after injection. Enhanced contrast in the tumor tissues was visualized for Gd-DOTA-G3-CLT1 at 2–60 min after injection. Contrast/noise ratios (CNRs) for Gd-DOTA-G3-CLT1 were 9, 10, 13, 15, 18, and 17 at 2, 5, 10, 15, 30, and 60 min after injection, respectively. The tumor CNRs for non-targeted Gd-DOTA-G3 reached a maximum of 11 at 15 min and declined to 7 at 60 min, and were significantly lower than those of Gd-DOTA-G3-CLT1 (P < 0.05). Both agents showed high CNRs (~100) in the blood in the heart at 2 min, which gradually decreased over time. Gd-DOTA-G3-CLT1 exhibited greater and prolonged CNR than Gd-DOTA-G3 in the blood (P < 0.05). Contrast enhancement in the urinary bladder gradually increased over time with both agents, which were readily excreted through glomerular filtration because of their small sizes (~6 nm). No blocking studies were performed.

Ex vivo biodistribution of Gd was performed in female nude mice (n = 3) bearing MDA-MB-231 xenografts at 48 min after injection of 0.03 mmol Gd/kg Gd-DOTA-G3-CLT1 or Gd-DOTA-G3 (8). The Gd retention for Gd-DOTA-G3-CLT1 was significantly higher than that of Gd-DOTA-G3 in the heart, kidney, liver, lung, skin, and tumor (P < 0.05). Both contrast agents were comparable in the spleen. The Gd contents were 5.8%, 5.0%, 4.8%, 2.4%, 2.4%, 1.2%, and 0.5% of injected dose of Gd-DOTA-G3-CLT1 per gram of tissue (ID/g) in the spleen, liver, kidney, heart, skin, lung, and muscle, respectively. The femur contained <0.1% ID/g. The tumor Gd contents were 2.4% ID/g and 0.3% ID/g for Gd-DOTA-G3-CLT1 and Gd-DOTA-G3, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+human)]

No publication is currently available.

## NIH Support

R01 CA097465

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
8 Tan M., Wu X., Jeong E.K., Chen Q., Lu Z.R. (2010). Peptide-targeted Nanoglobular Gd-DOTA monoamide conjugates for magnetic resonance cancer molecular imaging. Biomacromolecules.
9 Kaneshiro T.L., Jeong E.K., Morrell G., Parker D.L., Lu Z.R. (2008). Synthesis and evaluation of globular Gd-DOTA-monoamide conjugates with precisely controlled nanosizes for magnetic resonance angiography. Biomacromolecules.